# ^177^Lu-Labeled 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid-Tyr-cyclo(DAB-Arg-cyclo(Cys-Phe-D-Trp-Lys-Thr-Cys))

Chemical name: | ^177^Lu-Labeled 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid-Tyr-cyclo(DAB-Arg-cyclo(Cys-Phe-D-Trp-Lys-Thr-Cys))
Abbreviated name: | ^177^Lu-AM3
Synonym:
Agent Category: | Peptides
Target: | Somatostatin receptors (SSTRs)
Target Category: | Receptors
Method of detection: | Single-photon emission computed tomography (SPECT) and planar imaging
Source of signal / contrast: | ^177^Lu
Activation: | No
Studies: | - In vitro; - Rodents | For structures of octreotide analogues, click on PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance?term=octreotide).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=somatostatin+receptor+and+targeted)]

The ^177^Lu-labeled 1,4,7,10-tetraazacyclododecane-1,4,7,10-tetraacetic acid (DOTA)-Tyr-cyclo(DAB-Arg-cyclo(Cys-Phe-D-Trp-Lys-Thr-Cys)), abbreviated as ^177^Lu-AM3, is a somatostatin (SST)-based, bicyclic peptide conjugate developed by Fani et al. for SST receptor (SSTR)–targeted imaging of neuroendocrine tumors (1).

The human SSTR family is a group of G-protein–coupled receptors with five members (SSTR1–SSTR5). All receptor members have seven α-helical transmembrane domains and possess a highly conserved sequence motif (YANSCANPI/VLY) in the seventh topology, which serves as a signature sequence for this family (2-4). Overall, there is 39%–57% sequence identity among the members, with the highest homology between SSTR1 and SSTR4, and among SSTR2, SSTR3, and SSTR5, respectively. The two groups of receptors also differ in their interactions with SST and its analogs (3-6). SSTR2, SSTR3, and SSTR5 have a high affinity for octreotide and seglitide, whereas SSTR1 and SSTR4 exhibit a very low affinity for them. With the exception of SSTR2, the precise contributions of other members remain to be elucidated. This is largely due to the lack of highly selective ligands and the co-expression of different members in single cells. SSTRs are distributed widely in cells both in the nervous system and periphery, and they have been shown to be overexpressed in a large number of malignancies, with particularly high density in neuroendocrine tumors (2, 7, 8).

As the targets of SST radiopharmaceuticals, SSTRs are of considerable clinical relevance for tumor imaging and radionuclide therapy (2, 9, 10). Because the native SST has a very short biological half-life (<2 min), various analogs have been synthesized, including a group of bicyclic peptides. Bicyclic peptides were first synthesized to understand the bioactive conformation and pharmacophoric amino acid sequence, and to increase the metabolic stability of the natural peptide SST-14 (also known as somatotropin release-inhibiting factor (SRIF)-14) by increasing the rigidity of bicyclic peptides (11, 12). Thereafter, various modified bicyclic peptides have been synthesized and have exhibited higher potency and longer duration of biological activity than SRIF-14 (1, 11, 12). As seen in the structure of the lead peptide cyclo(Aha,cyclo(Cys-Phe-D-Trp-Lys-Thr-Cys)), conformational constraints are introduced by head-to-tail coupling of a 16-atom ring with 7-aminoheptanoic acid (Aha) to the N- and C-terminally amino acid–deleted octreotide. To identify metabolically stable pansomatostatin analogs, a group of investigators from Switzerland have generated a set of bicyclic peptides by forming a second 16-atom ring with Arg and γ-aminobutyric acid (GABA) while keeping the octreotide 20-atom sequence as an inner circle (13-15). These modifications led to development of another lead peptide, cyclo(Arg-cyclo(Cys-Phe-D-Trp-Lys-Thr-Cys)-GABA), which is named HR3005 (1). Arg has been shown to be important for broad binding to SSTR subtypes, and GABA can be exchanged with diaminobutyric acid (DAB) for chelator coupling. Based on the HR3005 sequence, four bicyclic analogs have been further synthesized by Fani et al. from the same group (1). The influence of the conformational constraints on receptor binding profiles and the pharmacokinetics of the respective radiopeptides have been investigated. Studies by Fani et al. have shown that the high rigidity of these bicyclic radiopeptides leads to agonistic ligands with good affinity for all five SSTRs (1). The pharmacokinetic data of the DOTA-conjugated bicyclic peptide AM3 (DOTA-Tyr-cyclo(DAB-Arg-cyclo(Cys-Phe-D-Trp-Lys-Thr-Cys))), make it an excellent candidate as an imaging radiotracer (1).

### Related Resource Links:

- MICAD chapters on SSTR imaging (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=somatostatin+receptor+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information on SSTRs (http://www.ncbi.nlm.nih.gov/gene/?term=somatostatin+receptors)
- Articles on SSTRs in Online Mendelian Inheritance in Man (OMIM (http://www.ncbi.nlm.nih.gov/omim?term=somatostatin%20receptors))
- Somatostatin analogs in PubChem (http://www.ncbi.nlm.nih.gov/sites/entrez?db=pccompound&term=somatostatin)
- Bioassays of SSTRs in PubChem (http://www.ncbi.nlm.nih.gov/pcassay?term=somatostatin%20receptors)
- SSTR-related clinical trials in ClinicalTrial.gov (http://clinicaltrials.gov/ct2/results?term=somatostatin+receptors)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=20956465)]

Fani et al. synthesized AM3 on the basis of the lead peptide HR3005 (1). The GABA in HR3005 was replaced with DAB, followed by coupling of the peptide with DOTA through Tyr as a spacer. The ^177^Lu-labeled AM3 (^177^Lu-AM3) was prepared by incubation of AM3 with ^177^LuCl_3_ at 95°C for 30 min in ammonium acetate buffer (pH 5.0). The radiotracer solution was prepared by dilution with 0.9% NaCl containing 0.1% bovine serum albumin. The overall yield was ~30%. The ^177^Lu-labeling yield was >97% with a specific activity of 17 GBq/µmol (0.46 Ci/µmol). The radiochemical purity of ^177^Lu-AM3 was >95%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=20956465)]

Fani et al. characterized AM3 and ^177^Lu-AM3 for their binding affinity, cell internalization, stimulating effect on intracellular Ca^2+^ release, and stability (1).

The binding profile of AM3 was determined with receptor autoradiography. The cell membrane pellets were prepared from human embryonic kidney (HEK) cells expressing different subtypes of SSTRs (16). The binding affinity was expressed as 50% inhibitory concentration (IC_50_; n > 3). The lead peptide HR3005 showed high affinity (comparable to SRIF-28) for SSTR2 (2.4 ± 0.6 nM) and SSTR3 (3.4 ± 0.8 nM), and moderate affinity for SSTR5 (14.5 ± 4.5 nM), SSTR1 (34 ± 10 nM), and SSTR4 (68 ± 22 nM), conferring almost pansomatostatin potency to this peptide. Replacement of GABA with DAB in the HR3005 did not change the affinity profile, whereas DOTA-coupling led to marked loss of affinity for all SSTR subtypes. By introducing Tyr as a spacer between DOTA and the peptide, the affinity of AM3 recovered to levels comparable to those of HR3005. The IC_50_ values of AM3 were 119 ± 6 nM for SSTR1, 2.3 ± 0.2 nM for SSTR2, 4.0 ± 0.03 nM for SSTR3, 97 ± 21 nM for SSTR4, and 27 ± 1 nM for SSTR5. The binding profile of ^177^Lu-AM3 was not examined.

The immunofluorescence microscopy–based internalization assay for SSTR2 and SSTR3 with HEK-SSTR2 and HEK-SSTR3 cells showed that unlabeled AM3 elicited a pronounced relocation of SSTR2 and SSTR3 from the plasma membrane to the cytoplasm at 30 min after it was applied to the cells, an effect similar to that of the control, SRIF-28.

The stimulating effect of AM3 on the intracellular Ca^2+^ release was tested with HEK cells expressing SSTR2, SSTR3, and SSTR5. Intracellular Ca^2+^ release is a part of the signal pathway regulated by native SST. On SSTR3 and SSTR5, no signal was found. On SSTR2, a large, concentration-dependent increase of the signal was observed. AM3 has been considered to be an agonist because of its stimulating effect on Ca^2+^ release and high potencies similar to those of SRIF-14. The agonist-elicited response in terms of the half maximal effective concentration value was 21.5 ± 3.5 nM.

The internalization rate and efflux of ^177^Lu-AM3 were studied with HEK-SSTR2 and HEK-SSTR3 cells. Internalization was expressed as percentage of the total applied radioactivity. In HEK-SSTR2 cells, 10.5 ± 1.2% of the ^177^Lu-AM3 was internalized at 4 h, and in HEK-SSTR3 cells, 15.3 ± 2.3% of the ^177^Lu-AM3 was internalized at 4 h. ^177^Lu-AM3 internalization reached a plateau in both HEK-SSTR2 and HEK-SSTR3 cells after 4 h. ^177^Lu-AM3 had a lower internalization rate than the reference molecule ^177^Lu-DOTATOC (23.8 ± 1.6% in HEK-SSTR2 cells). Nonspecific internalization was <1% (data not shown), indicating receptor-mediated internalization. The efflux of ^177^Lu-AM3 was found to be faster in HEK-SSTR2 cells than in HEK-SSTR3 cells. Within 4 h, 45%–50% of the ^177^Lu-AM3 was released from HEK-SSTR2 cells, whereas only ~35% was released from HEK-SSTR3 cells.

^177^Lu-AM3 was extremely stable in human blood and serum at 37°C. No metabolites were observed in the plasma and serum after 24 h and 7 days, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=20956465)]

Five-week-old athymic female Swiss nude mice with HEK-SSTR2 tumors in the right front leg and HEK-SSTR3 tumors in the other leg (n = 4–7 mice/group) were used for biodistribution studies after injection of ^177^Lu-AM3 (100 µl/10 pmol per 0.15 MBq (0.0041 mCi)) into the tail vein. Nonspecific uptake was determined with co-injection of 2,000-fold excess DOTANOC (17, 18). One group of mice was pre-injected with lysine 10 min before the injection of ^177^Lu-AM3 to study kidney blocking. The results were expressed as percentage of injected dose per gram of tissue (% ID/g).

^177^Lu-AM3 demonstrated fast blood clearance (only 0.01% ID/g was left at 4 h after injection), fast nontarget clearance, and high receptor-mediated uptake in the tumors. The kidneys were the only other tissue to accumulate radioactivity. At 1 h after injection, both tumors accumulated the greatest amount of ^177^Lu-AM3, with the SSTR3 tumors (12.74 ± 0.75% ID/g) exhibiting slightly higher uptake than the SSTR2 tumors (10.37 ± 0.76% ID/g). Four hours after injection, ~60% of the initially accumulated radioactivity remained in both tumors, with 7.56 ± 2.16% ID/g in the SSTR3 tumors and 6.05 ± 1.13% ID/g in the SSTR2 tumors. At 24 h after injection, <30% was tumor-bound. Blocking experiments with DOTANOC (high affinities for SSTR2, SSTR3, and SSTR5) confirmed the specific and receptor-mediated uptake, showing only 0.37 ± 0.07% ID/g in the SSTR3 tumors and 1.82 ± 0.66% ID/g in the SSTR2 tumors at 4 h after injection. The radioactivity in the kidneys was 7.81 ± 0.24% ID/g and 5.09 ± 1.10% ID/g at 1 h and 4 h, respectively. The kidney uptake was not affected by the blocking agent DOTANOC, indicating that this uptake is not receptor-mediated. The tumor/kidney ratio was >1 at 1 h after injection, but the slower washout from the kidneys resulted in decreasing tumor/kidney ratios with time. The SSTR2/kidney and SSTR3/kidney ratios were 1.3 and 1.6 at 1 h, respectively, and 0.8 and 1.2 at 24 h after injection, respectively. Pre-injection of lysine (20 mg/100 µl) resulted in ~50% reduction of the kidney uptake with no significant impact on the tumor uptake.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Fani M., Mueller A., Tamma M.L., Nicolas G., Rink H.R., Cescato R., Reubi J.C., Maecke H.R. (2010). Radiolabeled bicyclic somatostatin-based analogs: a novel class of potential radiotracers for SPECT/PET of neuroendocrine tumors. J Nucl Med.
2 Froidevaux S., Eberle A.N. (2002). Somatostatin analogs and radiopeptides in cancer therapy. Biopolymers.
3 Tulipano G., Schulz S. (2007). Novel insights in somatostatin receptor physiology. Eur J Endocrinol.
4 van der Hoek J., Hofland L.J., Lamberts S.W. (2005). Novel subtype specific and universal somatostatin analogues: clinical potential and pitfalls. Curr Pharm Des.
5 Lesche S., Lehmann D., Nagel F., Schmid H.A., Schulz S. (2009). Differential effects of octreotide and pasireotide on somatostatin receptor internalization and trafficking in vitro. J Clin Endocrinol Metab.
6 Yim C.B., Dijkgraaf I., Merkx R., Versluis C., Eek A., Mulder G.E., Rijkers D.T., Boerman O.C., Liskamp R.M. (2010). Synthesis of DOTA-conjugated multimeric [Tyr3]octreotide peptides via a combination of Cu(I)-catalyzed "click" cycloaddition and thio acid/sulfonyl azide "sulfo-click" amidation and their in vivo evaluation. J Med Chem.
7 Strowski M.Z., Blake A.D. (2008). Function and expression of somatostatin receptors of the endocrine pancreas. Mol Cell Endocrinol.
8 Kwekkeboom D.J., Kam B.L., van Essen M., Teunissen J.J., van Eijck C.H., Valkema R., de Jong M., de Herder W.W., Krenning E.P. (2010). Somatostatin-receptor-based imaging and therapy of gastroenteropancreatic neuroendocrine tumors. Endocr Relat Cancer.
9 Bal C.S., Gupta S.K., Zaknun J.J. (2010). Radiolabeled somatostatin analogs for radionuclide imaging and therapy in patients with gastroenteropancreatic neuroendocrine tumors. Trop Gastroenterol.
10 de Jong M., Breeman W.A., Kwekkeboom D.J., Valkema R., Krenning E.P. (2009). Tumor imaging and therapy using radiolabeled somatostatin analogues. Acc Chem Res.
11 Veber D.F., Holly F.W., Paleveda W.J., Nutt R.F., Bergstrand S.J., Torchiana M., Glitzer M.S., Saperstein R., Hirschmann R. (1978). Conformationally restricted bicyclic analogs of somatostatin. Proc Natl Acad Sci U S A.
12 Veber D.F., Freidlinger R.M., Perlow D.S., Paleveda W.J., Holly F.W., Strachan R.G., Nutt R.F., Arison B.H., Homnick C., Randall W.C., Glitzer M.S., Saperstein R., Hirschmann R. (1981). A potent cyclic hexapeptide analogue of somatostatin. Nature.
13 Ginj M., Hinni K., Tschumi S., Schulz S., Maecke H.R. (2005). Trifunctional somatostatin-based derivatives designed for targeted radiotherapy using auger electron emitters. J Nucl Med.
14 Ginj M., Schmitt J.S., Chen J., Waser B., Reubi J.C., de Jong M., Schulz S., Maecke H.R. (2006). Design, synthesis, and biological evaluation of somatostatin-based radiopeptides. Chem Biol.
15 Ginj M., Zhang H., Waser B., Cescato R., Wild D., Wang X., Erchegyi J., Rivier J., Macke H.R., Reubi J.C. (2006). Radiolabeled somatostatin receptor antagonists are preferable to agonists for in vivo peptide receptor targeting of tumors. Proc Natl Acad Sci U S A.
16 Reubi J.C., Schar J.C., Waser B., Wenger S., Heppeler A., Schmitt J.S., Macke H.R. (2000). Affinity profiles for human somatostatin receptor subtypes SST1-SST5 of somatostatin radiotracers selected for scintigraphic and radiotherapeutic use. Eur J Nucl Med.
17 Wild D., Macke H.R., Waser B., Reubi J.C., Ginj M., Rasch H., Muller-Brand J., Hofmann M. (2005). 68Ga-DOTANOC: a first compound for PET imaging with high affinity for somatostatin receptor subtypes 2 and 5. Eur J Nucl Med Mol Imaging.
18 Wild D., Schmitt J.S., Ginj M., Macke H.R., Bernard B.F., Krenning E., De Jong M., Wenger S., Reubi J.C. (2003). DOTA-NOC, a high-affinity ligand of somatostatin receptor subtypes 2, 3 and 5 for labelling with various radiometals. Eur J Nucl Med Mol Imaging.